# Methyl ester of 1-O-(4-(2-[^18^F]fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate

Chemical name: | Methyl ester of 1-O-(4-(2-[^18^F]fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate
Abbreviated name: | [^18^F]FEAnGA-Me
Synonym:
Agent Category: | Compound
Target: | β-Glucuronidase (β-GUS; βG)
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | Yes
Studies: | - In vitro; - Rodents | Click on above structure for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Glucuronidase&cmd=DetailsSearch)]

The β-glucuronidase (β-GUS; EC 3.2.1.31) is a lysosomal enzyme that catalyzes the hydrolysis of β-glucuronic acid residues from the cell-surface glycosaminoglycans for normal reconstruction of the extracellular matrix (ECM) (1), and the enzyme is believed to participate in the processes of angiogenesis, cancer metastasis, and inflammation (2). The β-GUS is known to activate prodrugs (PDs) for the treatment of cancer. β-GUS also has been used to track the path of gene delivery vehicles, and there is evidence that it can be used as a biomarker to detect cancerous tumors (3). Normal tissues have low levels of β-GUS in the ECM, but tissues under pathological stress, such as bacterial infection, fibrosis, and malignancy, show elevated levels of the enzyme (4). As a result of cell lysis, intracellular β-GUS is released from the necrotic parts of neoplastic tumors, and its activity in these lesions has been utilized for the in situ activation of anti-cancer PDs to treat cancers (1). Because chemotherapeutic anti-cancer drugs are non-selectively toxic to healthy cells, they are generally of limited efficacy to the patient due to their undesirable side effects on the normal biological systems. The conversion of a toxic drug into a non-toxic PD that can be activated only under specific conditions (e.g., by enzyme catalysis or chemical hydrolysis) would facilitate drug activation only in tissues that provide the specialized microenvironment and improve its concentration and efficacy at the desired location in the body (5, 6). For example, glucuronide PDs (drugs that are linked to a glucuronic acid moiety with or without a linker) have been shown to have superior anti-tumor activity compared with the parent drugs because the activated drugs are released from the PDs by the β-GUS activity in a site-specific manner (7, 8).

β-GUS activity varies among individuals, and its expression or accumulation in tumor tissues may change depending on the type of neoplasm or the location in the body (1, 9). Fluorescent or bioluminescent substrates were developed to determine the expression of β-GUS with optical imaging in the various tissues of mice (3). However, this imaging modality is suitable for the detection of fluorescence or bioluminescence signals generated only in the superficial tissues of small animals such as rodents; the low depth of light penetration in tissues is a limitation for its application in large animals and humans (1, 4, 10). Imaging modalities such as positron emission tomography (PET) and single-photon emission computed tomography (SPECT), which use radionuclides to generate tracer signals, can be used to detect and determine the activity of enzymes such as the β-GUS because signals generated by radiolabeled probes can be detected even in deep locations in the body (11). In general, PET imaging has a higher sensitivity than SPECT and has been used to investigate drug kinetics in preclinical and clinical settings (11).

Antunes et al. synthesized 1-O-(4-(2-[^18^F]fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-O-β-D-glucopyronuronate ([^18^F]-FEAnGA) as a PD in an effort to develop a probe that could be used with PET to detect and visualize β-GUS activity in tumors (1, 4) and inflamed tissues (1, 10) in rodents. The mechanism of in vitro/in vivo activation of [^18^F]-FEAnGA is described elsewhere (4). Although [^18^F]-FEAnGA could be used to detect β-GUS activity and distinguish cancerous tumors or inflamed tissues from the surrounding normal tissues, only low levels of radioactivity were detected in the tumorous or inflamed areas compared with the healthy tissues. The investigators concluded that the low accumulation of label in the lesions was due to the high hydrophilicity of the PD and its rapid clearance from the body through the kidneys (1). It has been shown that conversion of anti-cancer PDs to their methyl esters renders them considerably less hydrophilic and increases the circulation half-life of the PD because the methylated-PD first has to be demethylated by an esterase (to produce the PD) while in circulation before the active drug could be released from the PD by another enzyme(s) such as the β-GUS at the desired site(s) in the body (12). On the basis of these observations, a [^18^F]-fluoride-labeled methyl ester of FEAnGA was synthesized ([^18^F]-FEAnGA-Me) and evaluated for the imaging of β-GUS activity in a rodent tumor/inflammation model (12). Briefly, a carboxylesterase in the plasma hydrolyzes [^18^F]-FEAnGA-Me to [^18^F]-FEAnGA, which is a substrate for the β-GUS, and its subsequent hydrolysis by the enzyme results in the production of glucuronic acid, 4-hydroxy-3-nitrobenzyl alcohol (HNBA; acts as a spacer moiety in the intact [^18^F]-FEAnGA, and the concentration of this molecule in the reaction mixture can be measured with ultraviolet (UV) spectroscopy at 402 nm after the hydrolysis of FEAnGA), and 2-[^18^F]fluoroethylamine ([^18^F]-FEA). Subsequently, [^18^F]-FEA can be detected with PET imaging because it accumulates in the cells by passive diffusion (10).

### Related Resource Links

Other prodrug chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Prodrug+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Homo sapiens β-GUS protein and mRNA sequences (http://www.ncbi.nlm.nih.gov/nuccore/NM_000181.3)

Prodrug-related clinical trials (http://clinicaltrials.gov/ct2/results?term=prodrugs)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20synthesis&cmd=DetailsSearch)]

The synthesis of FEAnGA-Me and its labeling with [^18^F]-fluoride have been described by Antunes et al. (4, 12). The radiochemical yield (RCY) and radiochemical purity (RCP) of the labeled compound were reported to be 10 ± 5% (based on [^18^F]-fluoride) and 95%, respectively. The total time required for the synthesis and purification of the final labeled product was 120 min. [^18^F]-FEAnGA-Me was reported to have a specific activity of 185 ± 71 GBq/μmol (4.9 ± 1.9 Ci/μmol).

[^18^F]-FEAnGA was synthesized for use in studies, and the RCY and the RCP of this tracer were reported to be 10%–15% and >95%, respectively. The specific activity of [^18^F]-FEAnGA was 149 ± 33 GBq/μmol (4.0 ± 0.89 Ci/μmol) (12).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20in%20vitro%20studies&cmd=DetailsSearch)]

At least >95% of [^18^F]-FEAnGA-Me was intact in phosphate-buffered saline (pH not reported) after incubation for 1 h at 37°C as determined with radio-thin-layer chromatography (radio-TLC; the Rf values for FEA, FEAnGA, and FEAnGA-Me were 0.1, 0.4, and 1.0, respectively) (4, 12).

The lipophilicity (Log D) of [^18^F]-FEAnGA-Me in an n-octanol/water mixture was determined to be −0.58 ± 0.0002 at pH 7.4 (12) compared with −1.61 ± 0.01 for [^18^F]-FEAnGA at the same pH (4).

To study the in vitro hydrolysis of non-radioactive FEAnGA-Me in the presence of commercially available Escherichia coli β-GUS (74 U) and porcine liver carboxylesterase (15 U), the compound (200 μM) was incubated with the enzymes for 1 h at 37°C (12). Measurement of the amount of HNBA generated from the reaction showed that 80% of the compound was completely hydrolyzed at the end of the incubation. When [^18^F]-FEAnGA-Me was incubated with rat plasma, 99% of the radiolabeled compound was converted to [^18^F]-FEAnGA within 30 min (12). In another study, [^18^F]-FEAnGA-Me was incubated with rat plasma in the presence of E. coli β-GUS, and 50% of the tracer was reported to be hydrolyzed to [^18^F]-FEA within 30 min (12).

When C6 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-107&Template=cellBiology) rat glioma cells were incubated with [^18^F]-FEAnGA-Me in the presence of E. coli β-GUS and porcine liver carboxylesterase for 1 h, 60% of the radioactivity was determined to be associated with the cells at the end of the incubation (12). Radio-TLC analysis of the C6 cell growth medium revealed that 99% of [^18^F]-FEAnGA-Me was converted to [^18^F]-FEA in the presence of both the enzymes; however, in the presence of the β-GUS alone, only 7% of the radiochemical substrate was recovered as [^18^F]-FEA (12).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20rodentia&cmd=DetailsSearch)]

The use of [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA was compared for the PET imaging of C6 cell glioma tumors (right shoulder) and inflammation (induced with turpentine oil in the thigh of left hind leg) in the same rats (12). Anesthetized animals were intravenously injected with either [^18^F]-FEAnGA-Me (n = 6 rats) or [^18^F]-FEAnGA (n = 8 rats) through the penile vein, and 60-min PET scans of the tumors were initiated. PET scans of inflammation in the legs could not be acquired because of equipment limitations, and the presence of high levels of radioactivity in the bladder interfered with acquiring precise images of the inflamed tissues. In the PET images, [^18^F]-FEAnGA-Me was observed to generate a high background compared to [^18^F]-FEAnGA. Both tracers had similar time-activity curves and showed peak accumulation of label in the viable parts of the tumors at 1.5 min postinjection (p.i.), followed by an exponential decrease over time. The half-lives of [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA in the viable parts of the tumor were 16 ± 2 min and 24 ± 9 min, respectively. In addition, the area under the curve values for the tumors were 23 ± 6 and 20 ± 4 (P = 0.65) with [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA, respectively.

After completion of the PET scans, the ex vivo biodistribution of [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA was compared at 60 min p.i. by calculating the standardized uptake values (SUV) for radioactivity accumulated in the various tissues of the rodents as described by Antunes et al. (12). Both tracers were reported to have similar SUVs for the peripheral organs of the animals. With [^18^F]-FEAnGA-Me, the SUVs for the liver and kidneys were significantly (P < 0.05) higher (0.97 ± 0.29 and 3.13 ± 0.67, respectively) than with [^18^F]-FEAnGA (0.34 ± 0.09 and 1.03 ± 0.48, respectively). The SUVs obtained with [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA for the tumor, inflamed muscle, and normal muscle in the rats are presented in Table 1.

Table 1: Uptake of radioactivity from [ ^ 18 ^ F]-FEAnGA-Me and [ ^ 18 ^ F]-FEAnGA in tumor, inflamed muscle, and normal muscle ( 12 ).

Tracer | Tissue SUV | | | T/N ratio | I/N ratio
Tracer | Tumor | Muscle | | T/N ratio | I/N ratio
Tracer | Tumor | Inflamed | Normal | T/N ratio | I/N ratio
[ ^ 18 ^ F]-FEAnGA-Me | 0.13 ± 0.02 | 0.13 ± 0.05 | 0.08 ± 0.02 | 1.85 ± 0.23 | 1.48 ± 0.22
[ ^ 18 ^ F]-FEAnGA | 0.13 ± 0.03 | 0.07 ± 0.02 | 0.04 ± 0.01 | 3.53 ± 0.52* | 1.59 ± 0.19

SUV, standardized uptake value; T/N, tumor/normal tissue; I/N, inflamed tissue/normal tissue.

*P = 0.02.

Although the tumor SUVs with [^18^F]-FEAnGA-Me and [^18^F]-FEAnGA were similar (Table 1), the tumor/normal muscle ratio (T/N ratio) was significantly lower (P = 0.02) with [^18^F]-FEAnGA-Me (1.85 ± 0.23) than with [^18^F]-FEAnGA (3.53 ± 0.52). The lower T/N ratio observed with [^18^F]-FEAnGA-Me was due to the higher uptake of radioactivity in the normal muscle with this tracer compared with [^18^F]-FEAnGA (Table 1), and this was attributed to the nonspecific uptake of the tracer in the muscle tissue.

From these studies, the investigators concluded that the enzyme-based, two-step PD activation strategy they used with [^18^F]-FEAnGA-Me was not suitable for the visualization of tumors or inflammation with PET in rodents (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F-FEAnGA-Me%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Antunes I.F., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). In Vivo Evaluation Of 1-o-(4-(2-fluoroethyl-carbamoyloxymethyl)-2-nitrophenyl)-o-beta-d-glucopyronurona te: A Positron Emission Tomographic Tracer For Imaging beta-glucuronidase Activity In A Tumor/inflammation Rodent Model. Mol Imaging.
2 Gandhi N.S., Freeman C., Parish C.R., Mancera R.L. (2012). Computational analyses of the catalytic and heparin-binding sites and their interactions with glycosaminoglycans in glycoside hydrolase family 79 endo-beta-D-glucuronidase (heparanase). Glycobiology.
3 Cheng T.C., Roffler S.R., Tzou S.C., Chuang K.H., Su Y.C., Chuang C.H., Kao C.H., Chen C.S., Harn I.H., Liu K.Y., Cheng T.L., Leu Y.L. (2012). An activity-based near-infrared glucuronide trapping probe for imaging beta-glucuronidase expression in deep tissues. J Am Chem Soc.
4 Antunes I.F., Haisma H.J., Elsinga P.H., Dierckx R.A., de Vries E.F. (2010). Synthesis and evaluation of [18F]-FEAnGA as a PET Tracer for beta-glucuronidase activity. Bioconjug Chem.
5 Antunes I.F., Haisma H.J., de Vries E.F. (2008). Tumor-specific activation of prodrugs: is there a role for nuclear medicine?. Nucl Med Commun.
6 Huttunen K.M., Raunio H., Rautio J. (2011). Prodrugs--from serendipity to rational design. Pharmacol Rev.
7 Thomas M., Clarhaut J., Tranoy-Opalinski I., Gesson J.P., Roche J., Papot S. (2008). Synthesis and biological evaluation of glucuronide prodrugs of the histone deacetylase inhibitor CI-994 for application in selective cancer chemotherapy. Bioorg Med Chem.
8 Renoux B., Legigan T., Bensalma S., Chadeneau C., Muller J.M., Papot S. (2011). A new cyclopamine glucuronide prodrug with improved kinetics of drug release. Org Biomol Chem.
9 Tzou S.C., Roffler S., Chuang K.H., Yeh H.P., Kao C.H., Su Y.C., Cheng C.M., Tseng W.L., Shiea J., Harm I.H., Cheng K.W., Chen B.M., Hwang J.J., Cheng T.L., Wang H.E. (2009). Micro-PET imaging of beta-glucuronidase activity by the hydrophobic conversion of a glucuronide probe. Radiology.
10 Antunes I.F., Doorduin J., Haisma H.J., Elsinga P.H., van Waarde A., Willemsen A.T., Dierckx R.A., de Vries E.F. (2012). 18F-FEAnGA for PET of beta-Glucuronidase Activity in Neuroinflammation. J Nucl Med.
11 Willmann J.K., van Bruggen N., Dinkelborg L.M., Gambhir S.S. (2008). Molecular imaging in drug development. Nat Rev Drug Discov.
12 Antunes, I.F., H.J. Haisma, P.H. Elsinga, J.W. Sijbesma, A.V. Waarde, A.T. Willemsen, R.A. Dierckx, and E.F. de Vries, In vivo evaluation of [(18)F]FEAnGA-Me: a PET tracer for imaging beta-glucuronidase (beta-GUS) activity in a tumor/inflammation rodent model. Nucl Med Biol, 2012